# ^99m^Tc(CO)_3_-Anti-epidermal growth factor receptor nanobody 8B6

Chemical name: | ^99m^Tc(CO)_3_-Anti-epidermal growth factor receptor nanobody 8B6
Abbreviated name: | ^99m^Tc(CO)_3_-8B6, ^99m^Tc-8B6
Synonym:
Agent category: | Antibody fragment, nanobody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20)]

Epidermal growth factor (EGF) is a 53-amino acid growth factor (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels of expression lead to increased cell proliferation (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 (11), was labeled as ^111^In-trastuzumab (http://www.ncbi.nlm.nih.gov/books/NBK23144/) (12-14). C225, an anti-EGFR (HER1), mouse-human chimeric, monoclonal IgG_1_ antibody, also known as erbitux or cetuximab, was labeled as ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/books/NBK23305/) (15, 16) for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (17, 18). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies and exhibit efficient and specific tumor targeting (19-21). Anti-HER1 nanobody 8B6 was radiolabeled with ^99m^Tc using tricarbonyl chemistry (^99m^Tc-8B6) for noninvasive in vivo SPECT imaging of HER1 expression in tumors in mice (22).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), nanobody (http://www.ncbi.nlm.nih.gov/books?term=nanobody%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20synthesis)]

Nanobody 8B6 was produced as a hexahistidine-tagged protein in Escherichia coli (22). A solution of [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and 8B6 (pH 7–8) was incubated for 90 min at 60°C with a radiochemical yield of >90%. The specific activity, radiochemical purity, and stability of ^99m^Tc-8B6 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20in%20vitro)]

Flow cytometry analysis showed that 8B6 binding was correlated to HER1 expression in DU145 human prostate carcinoma (200,000 sites/cell) and A431 human epidermoid carcinoma (2,000,000 sites/cell) cell lines (22). The binding of ^99m^Tc-8B6 (10 pmol) to A431 cells was inhibited by >90% with 10 nmol unlabeled 8B6.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20rodentia)]

Huang et al. (22) performed ex vivo biodistribution studies of 35 MBq (1 mCi) ^99m^Tc-8B6 (0.67 nmol/mouse) in normal mice (n = 6) at 3 h after injection. The tissue with the highest radioactivity accumulation (percent injected dose/g (% ID/g)) was the kidney (141.3% ID/g), followed by the liver (19.6% ID/g), spleen (5.1% ID/g), lung (3.3% ID/g), small intestine (1.2% ID/g), heart (1.1% ID/g), muscle (0.8% ID/g), and brain (0.1% ID/g). The blood circulation half-life of ^99m^Tc-8B6 was ~ 1.5 h.

SPECT imaging analysis was performed in nude mice bearing A431 (n = 6) or DU145 (n = 5) tumors after injection of 116 MBq (3.1 mCi) (0.67 nmol)) ^99m^Tc-8B6 at 3 h after injection (22). The A431tumors (5.2 ± 0.1% ID/cm^3^) were clearly visualized (P < 0.001), along with the kidneys (53.6 ± 8.3% ID/cm^3^) and liver (15.6 ± 1.9% ID/cm^3^), but the DU145 tumors (1.8 ± 0.3% ID/cm^3^) were not. Tumor/background ratios were 7.4 and 3.2 for A431 and DU145 tumors, respectively. No blocking studies were performed with unlabeled 8B6.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=8B6%20nanobody%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
18 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
19 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
20 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
21 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
22 Huang L., Gainkam L.O., Caveliers V., Vanhove C., Keyaerts M., De Baetselier P., Bossuyt A., Revets H., Lahoutte T. (2008). SPECT imaging with 99mTc-labeled EGFR-specific nanobody for in vivo monitoring of EGFR expression. Mol Imaging Biol.